# Near-infrared fluorescence 1,1-dioctadecyl-3,3,3,3-tetramethylindotricarbocyanine iodide (DiR)-labeled macrophages for cell imaging

Chemical name: | Near-infrared fluorescence 1,1-dioctadecyl-3,3,3,3-tetramethylindotricarbocyanine iodide (DiR)-labeled macrophages for cell imaging
Abbreviated name: | DiR-labeled macrophages
Synonym: | DiR-labeled Mø, DiR-Mø, DiR-macrophages
Agent Category: | Cells
Target: | Inflammation
Target Category: | Others
Method of detection: | Near-infrared fluorescence optical imaging
Source of signal / contrast: | DiR
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cell+tracking+and+macrophages)]

Personalized diagnosis and treatment with allogenic or autologous cells are becoming a reality in the field of medicine (1, 2). Cytotoxic or engineered T cells (http://clinicaltrials.gov/ct2/results?term=cytotoxic+T+cells) are under clinical trial for the treatment of hematopoietic or other malignant diseases (3). Contrast agent–tagged macrophages (http://clinicaltrials.gov/ct2/results?term=macrophage+and+imaging) are used as cellular probes to image the early inflammatory processes in macrophage-rich conditions such as inflammation, atherosclerosis, and acute cardiac graft rejection (1, 4). The roles of stem cells (http://clinicaltrials.gov/ct2/results?term=stem+cell) are under intensive investigation in therapeutic and regenerative medicine such as regenerating cardiomyocytes, neurons, bone, and cartilage (2, 5). Genetically modified cells (http://clinicaltrials.gov/ct2/results?term=genetic+disorders+and+cells) are used to treat genetic disorders (6). With the promising results from these studies, a critical issue is how to monitor the temporal and spatial migration and homing of these cells, as well as the engraftment efficiency and functional capability of the transplanted cells in vivo (7-9). Histopathological techniques have only been used to obtain the information on the fate of implanted cells at the time of animal euthanization or via biopsy or surgery. To understand the temporal changes of cell location, viability, and functional status, cell imaging techniques have been introduced during the last few years. Cells of interest are labeled with reporter genes, fluorescent dyes, or other contrast agents that transform the tagged cells into cellular probes or imaging agents (10). There are three fundamentally different routes for labeling cells of interest (7, 8). One route is to label the cells through systemic contrast agent application, as seen in the systemic use of superparamagnetic iron oxides (SPIO), subsequent phagocytosis of the SPIO by macrophages, and accumulation in macrophage-rich lesions. The second route is to label the cells in situ by injecting contrast agents into the tissue area of interest to monitor target cell migration after phagocytosis. The more widely used route is to label the cells in vitro, which is achieved by in vitro incorporation of contrast agents or by transfecting one or more reporter genes into cells. Each labeling method has its own limitations.

In vivo optical cell imaging is a rapidly developing field in small animal imaging that depends on the use of reporter genes and fluorescent dyes (9). The Reporter gene–based approach is crucial for molecular imaging, but it strongly depends on the stable, persistent, and long-term expression of desired proteins. Long-term expression of the reporter genes may lead to host immune response and may carry on to the daughter cells in the proliferating population. The fluorescence-based approach is simple, cost-effective, and relatively sensitive, but issues of tissue-to-detector geometry, auto-fluorescence, and tissue absorption and scattering remain to be solved. Accurate quantification may only be possible when measurements are properly controlled and signals are normalized. Organic dyes are also less valuable for long-term cell tracking strategies. Nevertheless, the fluorescence-based approach is easily used for a variety of straightforward short-term labeling applications in cell imaging. In an attempt to noninvasively trace and monitor macrophages for better localization, visualization, and quantification of inflammation processes, Eisenblatter et al. developed a protocol for rapid and safe macrophage labeling with near-infrared fluorescent dye, and the investigators further tested the feasibility to image inflammation in a mouse granuloma inflammation model (1). Imaging results showed that the tagging of macrophages with the lipophilic tracer 1,1-dioctadecyl-3,3,3,3-tetramethylindotricarbocyanine iodide (DiR) allowed the noninvasive tracking of inflammatory cells for several days in vivo. DiR has an excitation spectrum of 750 nm and an emission spectrum of 782 nm.

### Relevant Resource Links

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cell+tracking+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Clinical trails (http://clinicaltrials.gov/ct2/results?term=macrophage+and+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cell+tracking+and+macrophages+and+optical+imaging)]

Macrophages were obtained from mouse bone marrow stem cell progenitors that were differentiated into macrophages in vitro (1, 4). Macrophages were then incubated with DiR-labeling solution for 5 min to achieve labeling. The labeling efficiency varied in the labeling intensity between different preparations of primary murine macrophages and between different concentrations of DiR. In general, the labeled fluorescence intensity increased gradually with increasing DiR concentrations up to 2 µl (19.7 µmol/L)/1 × 10^5^ cells, with a slight drop at the higher dye concentrations. The standard dose of DiR was then set to 2.0 µl/1 × 10^5^ cells for cell labeling. The amount of DiR per labeled macrophage was not reported. In the phantom experiments, as few as 10,000 cells distributed in 1 ml agarose gel could be detected easily with a near-infrared fluorescent scanner and an acquisition time of 3 s. Increasing numbers of labeled cells in the phantom resulted in a linear increase of signal intensity (data not shown). Co-culture of the DiR-labeled macrophages in a 1:1 ratio with T cells for 2 days resulted in <0.5% of the CD3-positive T cells exhibiting DiR fluorescence. The DiR-labeled macrophages were uniform, and the fluorescent signal was intense after 2 days. These results indicated that the DiR-labeled macrophages were stable and that there was no relevant transfer of the dye from macrophages to T cells.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cell+tracking+and+macrophages+and+optical+imaging)]

Vitality and functionality assays of the DiR-labeled macrophages showed that DiR staining did not result in a higher rate of apoptosis, nor did it reduce the ability of macrophages to adhere to plastic surfaces. The phagocytosis of complement-opsonized Leishmania major parasites was not compromised in labeled macrophages compared with control cells. Equal nitric oxide production was obtained between labeled and control macrophages in response to interferon-gamma and lipopolysaccharide (LPS), indicating that the activation of DiR-labeled macrophages was unaffected (1, 4). However, the relationship between the loaded DiR amount per macrophage and macrophage functionality was not described in detail.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cell+tracking+and+macrophages+and+optical+imaging)]

Eisenblatter et al. tested the DiR-labeled macrophages as an optical probe in mice bearing cutaneous granuloma induced with LPS-containing polyacrylamide gel (PAG) (1). DiR-labeled macrophages were injected intravenously 24 h before PAG pellet implantation. The mice were examined daily for 7 days after injection. The signal/noise ratio (SNR) was calculated as signal intensity of pellet/standard deviation of noise. Optical imaging revealed the homing of labeled macrophages in different body compartments including the liver, lung, and bone marrow. The control PAG pellets without LPS displayed slightly higher fluorescence signals than did the reference tissue (skin neck area). Inclusion of LPS in the pellets resulted in significantly higher SNRs (529 ± 292 at 72 h after injection) than the control pellets (314 ± 168 at 72 h) (P < 0.05, n = 5). Tomographic imaging showed that the DiR-labeled macrophages distributed mainly in the periphery of the pellets, with a fluorescence signal in LPS-containing pellets ~2.7 times higher than in controls (459 ± 295 versus 253 ± 168; P < 0.05, n = 10). The injection of increasing numbers of labeled macrophages resulted in significantly increased signal intensities, presenting an almost linear correlation between tomographic signal intensity and the number of injected cells.

To verify extravasation and to quantify the number of DiR-stained macrophages inside the pellets, mice were euthanized and infiltrated cells in pellets were separated. Up to 27% of the 1 × 10^7^ injected cells could be recovered from the pellets. In agreement with the tomographic imaging data, increasing numbers of injected DiR-labeled macrophages resulted in increasing numbers of DiR-positive cells recovered from the pellets. Up to 23% of the recovered cells were DiR-positive macrophages. The DiR-positive cells were uniformly positive for the macrophage differentiation marker F4/80 and the macrophage colony-stimulating factor receptor (data not shown). The DiR- and F4/80-negative cells were exclusively granulocytes. There was no evidence that in vivo macrophages lost their label to other cells (granulocytes) during the observation period. On the basis of the results, ~5 × 10^5^ cells had to be distributed in the pellet to provide a strong signal for the inflammation visualization with optical imaging (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Eisenblatter M., Ehrchen J., Varga G., Sunderkotter C., Heindel W., Roth J., Bremer C., Wall A. (2009). In vivo optical imaging of cellular inflammatory response in granuloma formation using fluorescence-labeled macrophages. J Nucl Med.
2 Mathiasen A.B., Haack-Sorensen M., Kastrup J. (2009). Mesenchymal stromal cells for cardiovascular repair: current status and future challenges. Future Cardiol.
3 Cesco-Gaspere M., Morris E., Stauss H.J. (2009). Immunomodulation in the treatment of haematological malignancies. Clin Exp Med.
4 Ehrchen J., Helming L., Varga G., Pasche B., Loser K., Gunzer M., Sunderkotter C., Sorg C., Roth J., Lengeling A. (2007). Vitamin D receptor signaling contributes to susceptibility to infection with Leishmania major. FASEB J.
5 Kuhn N.Z., Tuan R.S. (2010). Regulation of stemness and stem cell niche of mesenchymal stem cells: implications in tumorigenesis and metastasis. J Cell Physiol.
6 Bachoud-Levi A.C. (2009). Neural grafts in Huntington's disease: viability after 10 years. Lancet Neurol.
7 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
8 Hoehn M., Wiedermann D., Justicia C., Ramos-Cabrer P., Kruttwig K., Farr T., Himmelreich U. (2007). Cell tracking using magnetic resonance imaging. J Physiol.
9 Arbab A.S., Janic B., Haller J., Pawelczyk E., Liu W., Frank J.A. (2009). In Vivo Cellular Imaging for Translational Medical Research. Curr Med Imaging Rev.
10 Loebinger M.R., Kyrtatos P.G., Turmaine M., Price A.N., Pankhurst Q., Lythgoe M.F., Janes S.M. (2009). Magnetic resonance imaging of mesenchymal stem cells homing to pulmonary metastases using biocompatible magnetic nanoparticles. Cancer Res.